# ^111^In-Diethylenetriamine pentaacetic acid-human anti-insulin-like growth factor 1 receptor monoclonal antibody R1507

Chemical name: | ^111^In-Diethylenetriamine pentaacetic acid-human anti-insulin-like growth factor 1 receptor monoclonal antibody R1507
Abbreviated name: | ^111^In-DTPA-R1507, ^111^In-R1507
Synonym:
Agent category: | Antibody
Target: | Insulin-like growth factor 1 receptor (IGF-1R)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507)]

Insulin-like growth factor 1 (IGF-1, 70 amino acids) is secreted by the liver and target tissues in response to growth hormone stimulation (1). IGF-1 plays an important role in cell growth and development. IGF-1 binds to IGF-1 receptor (IGF-1R) with ~1,000-fold higher affinity than to insulin receptor. IGF-1R is a transmembrane tyrosine kinase receptor and is also highly expressed in many human cancers (2). IGF-1R plays an important role in tumor proliferation, apoptosis, angiogenesis, and metastasis (3, 4). Triple negative breast tumors are negative for estrogen receptors, progesterone receptors, and HER2. Patients with triple negative breast tumors have a lower survival rate than patients with estrogen receptor- or HER2-positive breast tumors (5). IGF-1R is overexpressed in 36% of all triple negative breast carcinomas (6).Therefore, monitoring of IGF-1R expression in breast tumor lesions with a non-invasive imaging modality is important for development of therapeutic treatments of these patients with anti-IGF-1R monoclonal antibodies (7). The human anti-IGF-1R monoclonal antibody R1507 is directed against the extracellular domain of human IGF-1R (8). In this chapter, Heskamp et al. (9) radiolabeled the human anti-IGF-1R monoclonal antibody R1507 with ^111^In for in vivo imaging of IFG-1R expression with single-photon emission computed tomography (SPECT). ^111^In-Diethylenetriamine pentaacetic acid-human anti-IGF-1R monoclonal antibody R1507 (^111^In-DTPA-R1507) has been evaluated in a triple negative breast cancer model in mice.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=IGF-1%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (IGF-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=3480)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (IGF-1R (http://www.ncbi.nlm.nih.gov/omim/147370))
- Clinical trials (IGF-1R (http://www.clinicaltrials.gov/ct2/results?term=IGF1R))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20synthesis)]

R1507 was conjugated with 10-fold molar excess of isothiocyanatobenzyl-DTPA in 0.1 M NaHCO3 (pH 9) for 60 min at room temperature (9). A solution of 244 MBq (6.6 mCi) ^111^InCl_3_ and 0.15 nmol DTPA-R1507 was incubated in buffer (pH 5–6) for 30 min at room temperature. ^111^In-DTPA-R1507 was purified with column chromatography. ^111^In-DTPA-R1507 exhibited a radiochemical purity of >98% with a labeling efficiency of >95%. The immunoreactivity of ^111^In-DTPA-R1507 was 99%. The number of DTPA groups per antibody was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20in%20vitro)]

Heskamp et al. (9) reported that the parent antibody R1507 exhibited 50% inhibitory concentration (IC_50_) values of 0.08–0.12 nM for IGF-1R on the triple negative human breast cancer cell line SUM149. ^111^In-DTPA-R1507 was mainly membrane-bound in the early hours of incubation and then was gradually internalized until 62% of the surface-bound radioactivity was internalized at 48 h after incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20rodentia)]

Heskamp et al. (9) performed ex vivo biodistribution studies in nude mice (n = 6/group) bearing the triple negative breast SUM149 xenografts with injection of 0.2 MBq (0.005 mCi, 3.3 pmol) ^111^In-DTPA-R1507 and co-injection with 6.6 pmol to 6.6 nmol unlabeled R1507. The optimal doses of R1507 for radioactivity accumulation in the tumors were 6.6 pmol and 19.8 pmol at 3 d after injection with 38% and 35% injected dose/gram (ID/g), respectively. For doses of 66 pmol or higher, tumor accumulation was <15% ID/g. The blood and muscle concentrations were ~15% ID/g and ~1% ID/g, respectively, at all doses. All the other major organs showed <10% ID/g at all doses. Therefore, only the tumors showed specific binding. In another experiment, 0.4 MBq (0.11 mCi) ^111^In-DTPA-R1507 (3.3 pmol) showed tumor accumulation of 20 ± 6% ID/g, 33 ± 6% ID/g, and 31 ± 4% ID/g at 1, 3, and 7 d after injection, respectively. Co-injection of 3.3 nmol R1507 reduced the tumor uptake to 5.6% ID/g at 7 d. The tumor/blood (3.8) and tumor/liver (12) ratios were highest at 7 d. In comparison, ^125^I-R1507 showed the highest tumor/blood (0.7) and tumor/liver (3.3) ratios at 3 d with a tumor uptake of 7% ID/g.

SPECT imaging in nude mice (n = 5) with 17.2 MBq (0.46 mCi, 10.4 pmol) ^111^In-DTPA-R1507 visualized the SUM149 tumor as early as 24 h after injection with a maximum contrast at 7 d. The tumor/liver ratio increased from 1.9 at 1 d to 5.8 at 7 d. Co-injection with excess R1507 (6.6 nmol) prevented the visualization of the tumor with the tumor/liver ratio of 1.5 at 7 d. Non-specific accumulation was observed in the liver, spleen, and salivary glands.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20human)]

No publication is currently available.

## References

1 Hernandez-Sanchez C., Blakesley V., Kalebic T., Helman L., LeRoith D. (1995). The role of the tyrosine kinase domain of the insulin-like growth factor-I receptor in intracellular signaling, cellular proliferation, and tumorigenesis. J Biol Chem.
2 LeRoith D., Werner H., Neuenschwander S., Kalebic T., Helman L.J. (1995). The role of the insulin-like growth factor-I receptor in cancer. Ann N Y Acad Sci.
3 Rosenzweig S.A., Atreya H.S. (2010). Defining the pathway to insulin-like growth factor system targeting in cancer. Biochem Pharmacol.
4 Baserga R., Hongo A., Rubini M., Prisco M., Valentinis B. (1997). The IGF-I receptor in cell growth, transformation and apoptosis. Biochim Biophys Acta.
5 Carey L.A., Dees E.C., Sawyer L., Gatti L., Moore D.T., Collichio F., Ollila D.W., Sartor C.I., Graham M.L., Perou C.M. (2007). The triple negative paradox: primary tumor chemosensitivity of breast cancer subtypes. Clin Cancer Res.
6 Lerma E., Peiro G., Ramon T., Fernandez S., Martinez D., Pons C., Munoz F., Sabate J.M., Alonso C., Ojeda B., Prat J., Barnadas A. (2007). Immunohistochemical heterogeneity of breast carcinomas negative for estrogen receptors, progesterone receptors and Her2/neu (basal-like breast carcinomas). Mod Pathol.
7 Zha J., O'Brien C., Savage H., Huw L.Y., Zhong F., Berry L., Lewis Phillips G.D., Luis E., Cavet G., Hu X., Amler L.C., Lackner M.R. (2009). Molecular predictors of response to a humanized anti-insulin-like growth factor-I receptor monoclonal antibody in breast and colorectal cancer. Mol Cancer Ther.
8 Gong Y., Yao E., Shen R., Goel A., Arcila M., Teruya-Feldstein J., Zakowski M.F., Frankel S., Peifer M., Thomas R.K., Ladanyi M., Pao W. (2009). High expression levels of total IGF-1R and sensitivity of NSCLC cells in vitro to an anti-IGF-1R antibody (R1507). PLoS One.
9 Heskamp S., van Laarhoven H.W., Molkenboer-Kuenen J.D., Franssen G.M., Versleijen-Jonkers Y.M., Oyen W.J., van der Graaf W.T., Boerman O.C. (2010). ImmunoSPECT and immunoPET of IGF-1R expression with the radiolabeled antibody R1507 in a triple-negative breast cancer model. J Nucl Med.